# 3'-Deoxy-3'-[^18^F]fluoro-1-β-D-xylofuranosyl-adenine

Chemical name: | 3'-Deoxy-3'-[^18^F]fluoro-1-β-D-xylofuranosyl-adenine
Abbreviated name: | [^18^F]FXA
Synonym:
Agent Category: | Compound
Target: | Unknown
Target Category: | Non-catabolized trapping inside cells
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine)]

Adenylates are important in cellular metabolism and functions (1). Adenosine is converted intracellularly to adenosine triphosphate (ATP), which is an important source of energy as well as a regulator of cellular functions. Adenosine stimulates the acetylcholine-sensitive K^+^ current in the heart. Many fluorinated analogs of adenosine nucleoside have been investigated as potential antitumor and antiviral agents (2-5). 3'-Deoxy-3'-fluoro-9-β-D-xylofuranosyl-adenine (FXA) was found to have antiviral activity (3, 6). [^18^F]FXA has been synthesized and studied in tumor-bearing mice with positron emission tomography (PET) imaging. [^18^F]FXA was not visualized in the tumor but in the heart (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+synthesis)]

Alauddin et al. (7) synthesized [^18^F]FXA by reaction of the respective triflate (N3,2’,5’-tri-methoxytrityl-3’-trifluoromethanesulfonyl-9-β-D-arabinofuranosyl-adenine with tetrabutylammonium [^18^F]fluoride, followed by acid hydrolysis to remove the methoxytrityl protecting groups. The desired product, [^18^F]FXA, was purified with high-performance liquid chromatography with a radiochemical yield of 30%–35% (decay-corrected) and a radiochemical purity >99%. The average specific activity for [^18^F]FXA was >74 GBq/µmol (2,000 mCi/µmol) at the end of the synthesis. Total synthesis time was 90–95 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+rodentia)]

Alauddin et al. (7) performed biodistribution studies of [^18^F]FXA in nude mice (n = 5) bearing an HT-29 tumor in the left flank and a herpes simplex virus thymidine kinase (HSV-tk)–transduced HT-29 tumor in the right flank. [^18^F]FXA cleared rapidly from the blood within 20 min after injection with a plasma half-life of ~8 min. The heart had the highest accumulation at 120 min (the only time point studied) with 8.4% injected dose (ID)/g, followed by the liver (6.9% ID/g) and kidney (6.4% ID/g). The accumulation in the two tumors was 0.67% ID/g in the wild-type tumor and 0.49% ID/g in the HSV-tk–transduced tumor, which suggests that [^18^F]FXA is not a substrate for HSV-tk gene. Radioactivity levels in the blood and muscle were 1.03% ID/g and 2.43% ID/g, respectively. The heart/blood ratio was 8.15. The tumor/blood ratio was <1, which suggests that [^18^F]FXA is not suitable for tumor imaging. PET images were obtained at 30, 60, and 120 min after injection. The heart exhibited the highest radioactivity, followed by the liver and kidney. Neither tumor was clearly visualized. No significant differences in images were observed at the three time points. No blocking experiment was performed. The authors suggested that further studies are necessary to understand the mechanism of heart accumulation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+2-fluoroadenosine+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-fluoroadenosine+human)]

No publication is currently available.

## NIH Support

CA72896

## References

1 Dzeja P.P., Terzic A. (2003). Phosphotransfer networks and cellular energetics. J Exp Biol.
2 Kim C.G., Yang D.J., Kim E.E., Cherif A., Kuang L.R., Li C., Tansey W., Liu C.W., Li S.C., Wallace S., Podoloff D.A. (1996). Assessment of tumor cell proliferation using [18F]fluorodeoxyadenosine and[18F]fluoroethyluracil. J Pharm Sci.
3 Mikhailopulo I.A., Poopeiko N.E., Pricota T.I., Sivets G.G., Kvasyuk E.I., Balzarini J., De Clercq E. (1991). Synthesis and antiviral and cytostatic properties of 3'-deoxy-3'-fluoro- and 2'-azido-3'-fluoro-2',3'-dideoxy-D-ribofuranosides of natural heterocyclic bases. J Med Chem.
4 Pittillo R.F., Moncrief C., Brockman R.W., Chambers P. (1964). Antimicrobial Activity of 2-Fluoroadenosine and 2-Fluoroadenine. Antimicrobial Agents Chemother (Bethesda).
5 Secrist J.A., Shortnacy A.T., Montgomery J.A. (1988). Synthesis and biological evaluations of certain 2-halo-2'-substituted derivatives of 9-beta-D-arabinofuranosyladenine. J Med Chem.
6 Van Aerschot A., Herdewijn P., Janssen G., Cools M., De Clercq E. (1989). Synthesis and antiviral activity evaluation of 3'-fluoro-3'-deoxyribonucleosides: broad-spectrum antiviral activity of 3'-fluoro-3'-deoxyadenosine. Antiviral Res.
7 Alauddin M.M., Shahinian A., Park R., Tohme M., Fissekis J.D., Conti P.S. (2007). Biodistribution and PET imaging of [(18)F]-fluoroadenosine derivatives. Nucl Med Biol.